# ^99m^Tc-Hydrazinonicotinic acid-single-chain Cys-tagged vascular endothelial growth factor-121

Chemical name: | ^99m^Tc-Hydrazinonicotinic acid-single-chain Cys-tagged vascular endothelial growth factor-121
Abbreviated name: | ^99m^Tc-HYNIC-scVEGF_121_
Synonym:
Agent Category: | Polypeptide
Target: | VEGF receptors
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (1).

VEGF receptors were found to be overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (6-8). Cys-tag, a fusion tag comprising 15 amino acids, was developed for site-specific conjugation via the free sulfhydryl group of Cys. Backer et al. (9) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain fragments (amino acid sequence 3–112 ) of VEGF_121_ joining head-to-tail to express as scVEGF, which can be labeled as ^64^Cu-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA)-scVEGF (^64^Cu-DOTA-scVEGF), ^99m^Tc-hydrazinonicotinic acid (HYNIC)-scVEGF (^99m^Tc-HYNIC-scVEGF), and Cy5.5-scVEGF for imaging VEGFR expression to study tumor angiogenesis (10). ^99m^Tc-HYNIC-scVEGF is being developed for single-photon emission computed tomography (SPECT) imaging of VEGFR-2 in tumor vasculature.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+synthesis)]

Backer et al. (9) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain fragments (amino acid sequence 3–112) of VEGF_121_ joining head-to-tail to express as scVEGF in Escherichia coli. ^99m^Tc labeling of scVEGF was performed through HYNIC chelation (10). A mixture of scVEGF and HYNIC-maleimide in a molar ratio of 1:3 was incubated at room temperature for 60 min. The HYNIC-scVEGF conjugate was purified with column chromatography. The number of HYNIC molecules per protein was ~1. For radiolabeling, scVEGF was added to a ^99m^Tc-tricine complex. The reaction mixture was incubated at 55ºC for 1 h. ^99m^Tc-HYNIC-scVEGF was purified with column chromatography. ^99m^Tc-HYNIC-inVEGF, an inactive control, was prepared by conjugation of 7–8 biotins to ^99m^Tc-HYNIC-scVEGF.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+and+in+vitro)]

In vitro competition binding studies were performed in 293/KDR cells expressing cloned human VEGFR-2 in competition with the chimeric toxin SLT-VEGF for binding to VEGFR-2 (10). ^64^Cu-DOTA-PEG-scVEGF, DOTA-PEG-scVEGF, HYNIC-scVEGF, and Cy5.5-scVEGF inhibited the binding of SLT-VEGF to VEGFR-2. DOTA-PEG-scVEGF, HYNIC-scVEGF, and Cy5.5-scVEGF stimulated tyrosine phosphorylation of VEGFR-2 in 293/KDR cells in a manner similar to VEGF.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+rodentia)]

Backer et al. (10) performed biodistribution studies of ^99m^Tc-HYNIC-scVEGF and ^99m^Tc-HYNIC-inVEGF in mice bearing 4T1 murine breast tumors expressing VEGFR-2. The tumor accumulated ~3% injected dose per gram (% ID/g), whereas the muscle accumulated <0.5% ID/g. The organs with the highest accumulation of ^99m^Tc-HYNIC-scVEGF were the kidneys (~120% ID/g), lung (~6% ID/g), and liver (~6% ID/g) at 1 h after injection. ^99m^Tc-HYNIC-scVEGF was cleared from the blood rapidly with ~2% ID/g at 50 min. ^99m^Tc-HYNIC-scVEGF remained >95% intact at 3 and 50 min in the blood. PET imaging studies were performed at 1 h after injection of ^99m^Tc-HYNIC-scVEGF or ^99m^Tc-HYNIC-inVEGF. ^99m^Tc-HYNIC-scVEGF revealed higher and more heterogeneous focal accumulation than ^99m^Tc-HYNIC-inVEGF. Tumor/soft tissue ratio was 10–15 for ^99m^Tc-HYNIC-scVEGF. Autoradiography of the tumor sections showed that ^99m^Tc-HYNIC-scVEGF accumulated mainly at the outer rim of the tumor. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF+human)]

No publication is currently available.

## NIH Support

R21 EB001946, R43 CA113080, P50 CA114747, CA064436

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Backer M.V., Patel V., Jehning B.T., Claffey K.P., Backer J.M. (2006). Surface immobilization of active vascular endothelial growth factor via a cysteine-containing tag. Biomaterials.
10 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.